# ^64^Cu-1,4,7,10-Tetraazacyclodecane-N,N',N'',N'''-tetraacetic acid-vascular endothelial growth factor

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclodecane-N,N',N'',N'''-tetraacetic acid- vascular endothelial growth factor
Abbreviated name: | ^64^Cu-DOTA-VEGF
Synonym: | ^64^Cu-DOTA-VEGF_121_, ^64^Cu-VEGF, ^64^Cu-VEGF_121_
Agent Category: | Peptide
Target: | Vascular endothelial growth factor receptors (VEGFR or VEGF receptors)
Target Category: | Receptor binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71051581), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001025368.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=7422) for more information about VEGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2864Cu-VEGF%29%20OR%20%28Vascular%20Endothelial%20Growth%20Factor%20for%20PET%29)]

^64^Cu-1,4,7,10-Tetraazacyclodecane-N,N',N'',N'''-tetraacetic acid (DOTA)-vascular endothelial growth factor (^64^Cu-DOTA-VEGF) is a radiolabeled molecular imaging agent developed for positron emission tomography (PET) imaging of tumor angiogenesis and guiding antiangiogenic treatment (1). ^64^Cu is a positron emitter with a half-life (t_½_) of 12.7 h.

Angiogenesis is a process of development and growth of new blood vessels from pre-existing vessels (2). Tumor growth depends on the formation of new blood vessels from this process. Normal angiogenesis is orderly and highly regulated, whereas tumor angiogenesis is chaotic and irregular. Abnormal angiogenesis is important in the carcinogenesis, growth and progression of human solid and hematologic tumors (3). VEGF is both a vascular growth factor and a vascular permeability factor, and it plays a central and critical role in the regulation of angiogenesis (4). VEGF induces proliferation, sprouting, migration, and tube formation of endothelial cells (5). Different forms of VEGF bind to receptors that exhibit a tyrosine-kinase activity (2). VEGF and VEGF receptors (VEGFR) have been shown to be upregulated in many tumors.

VEGF is a dimeric glycoprotein of 36−46 kDa that has been implicated in several steps throughout the process of angiogenesis (3). The VEGF family currently consists of 6 growth factors and 3 high-affinity tyrosine-kinase receptors. The specific action of VEGF on the endothelial cells is mainly regulated by VEGFR1 and VEGFR2 (2). VEGF-A is the most well characterized member of the VEGF family and is composed of at least 7 isoforms due to alternative gene splicing. Located at chromosome 6p21.3, VEGF-A is encoded by 8 exons separated by 7 introns. These forms differ mainly in their bioavailability and can be characterized by heparin and heparin-sulfate binding domains encoded by exons 6 and 7. VEGF_121_ (121 amino acids) and VEGF_165_ (165 amino acids) isoforms have been shown to induce mitogenic and permeability-enhancing activity on endothelial cells. VEGF gene expression is upregulated by many stimuli and hormones. In cancer, VEGF is upregulated by the genetic events leading to malignant transformation. VEGF and its receptors are overexpressed in a variety of solid tumors (1).

Molecular imaging of angiogenesis offers serial non-invasive evaluation of various tumor parameters (6) PET imaging with the appropriate radiolabeled tracer targeted to angiogenic signaling pathways may allow the evaluation of specific aspects of tumor vascular biology. VEGF has been labeled with ^111^In, ^123^I and ^99m^Tc as potential Single Photon Emission Tomography imaging agents (7). Cai et al. (1) prepared the first PET agent for imaging VEGF by labeling VEGF_121_ with ^64^Cu.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2864Cu-VEGF%29%20OR%20%28Vascular%20Endothelial%20Growth%20Factor%20for%20PET%29%29%20AND%20synthesis)]

Cai et al. (1) cloned and sequenced gene for VEGF_121_ by polymerase chain reaction from human umbilical vein endothelial cells. The gene was inserted into the pET-32 vector downstream from the cleavable His_6_ tag sequence. Bacterial cells were transformed and positive clones were selected for optimal protein expression. The protein was isolated and the His_6_ tag was cleaved from VEGF_121_. The final protein was purified and concentrated.

^64^Cu labeling of VEGF_121_ was performed through DOTA chelation (1, 8). DOTA was obtained commercially and activated by 1-ethyl-3-[3-(dimethylamino)-propyl] carbodiimide (EDC) and N-hydroxysulfonosuccimide (SNHS) at pH 5.5 for 30 min with a molar ratio of 10:5:4 (DOTA/EDC/SNHS). Without purification, the DOTA-hydroxysulfosuccinimidyl was cooled to 4ºC and added to VEGF_121_. The reaction mixture was adjusted to pH 8.5 with 0.1 N of sodium hydroxide and allowed to incubate overnight at 4º C. The DOTA-VEGF_121_ conjugate was purified by a PD-10 column and concentrated. The final concentration was determined by ultraviolet absorbance at 280 nm. The number of DOTA molecules per VEGF_121_ molecule was 4.3 ± 0.2 (n = 3). For radiolabeling, about 20 μg of this conjugate was added to 74 MBq (2.47 mCi) of ^64^Cu chloride diluted in 300 μl of 0.1mol/L sodium acetate buffer. The reaction mixture was incubated for 1 h at 40ºC with constant shaking. ^64^Cu-DOTA-VEGF_121_ was purified by chromatography. The ^64^Cu labeling time, including the final purification was 90 ± 10 min (n = 5), and the radiolabeling yield was 87.4 ± 3.2%. The specific activity was 3.2 ± 0.1 GBq/mg (86.5 ± 2.7 mCi/mg). The radiochemical purity was >98%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2864Cu-VEGF%29%20OR%20%28Vascular%20Endothelial%20Growth%20Factor%20for%20PET%29%29%20AND%20in%20vitro)]

Cai et al. (1) used ^125^I-VEGF_165_ as the radioligand to perform cell binding assays of VEGF_121_ and DOTA-VEGF_121_ to PAE/KDR endothelial cells expressing VEGFR2. The 50% inhibitory concentrations (IC_50_) were 1.02 nmol/L and 1.66 nmol/L for VEGF_121_ and DOTA-VEGF_121_, respectively_._ Stability studies of incubating ^64^Cu-DOTA-VEGF_121_ in complete mouse serum at 37ºC showed no significant metabolite peak by high-performance liquid chromatography up to 24 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2864Cu-VEGF%29%20OR%20%28Vascular%20Endothelial%20Growth%20Factor%20for%20PET%29%29%20AND%20rodentia)]

MicroPET imaging studies of ^64^Cu-DOTA-VEGF_121_ were performed in mice bearing U87MG human glioblastomas. Each mouse received 5−10 MBq (0.14−0.27 mCi) of radioactivity in ~2−4 μg of VEGF_121_. The radioactivity uptake was rapid and high in small tumors (tumor volume = 64.9 ± 24.6 mm^3^, n = 3) with high VEGFR expression. The radioactivity levels measured as percentage of injected dose per g (% ID/g) were 14.9 ± 0.7, 16.3 ± 0.7, 16.3 ± 0.6, and 15.1 ± 0.8 at 2, 4, 16, and 23 h, respectively. The tumor was clearly visible as early as 1 h after injection. In comparison, the radioactivity uptake in the large tumors (tumor volume = 1,164.3 ± 179.6 mm^3^, n = 3) with low VEGFR expression was very low at all time points. The radioactivity levels were ~3−4% ID/g and ~1−2% ID/g at the peripheral region and the necrotic center, respectively. The radioactivity levels were high in the kidney (33.0 ± 13.5% ID/g at 2 h) and liver (17.1 ± 3.2% ID/g at 2 h) in both groups of mice bearing small and large tumors. These radioactivity levels dropped steadily over time. All other organs exhibited very low radioactivity levels. Biodistribution studies of mice at 23 h after administration confirmed that the PET quantification was a true reflection of organ radioactivity levels.

Blocking experiments were performed to test the specificity of ^64^Cu-DOTA-VEGF_121_ in the group of mice bearing small tumors (1). A dose of 100 μg of unlabeled VEGF_121_ was injected into each mouse 30 min before the administration of ^64^Cu-DOTA-VEGF_121_. PET imaging showed the radioactivity uptake appeared to be noticeably lower than that of mice without blocking. The radioactivity levels in the tumor were significantly lower at all time points. Extrapolated from the figure in the article, the radioactivity levels (% ID/g) in small tumors with blocking were estimated to be ~9 (2 h), ~10 (4 h), ~11 (16 h), and ~10 (23 h), respectively.

Immunofluorescence staining and Western blot of tumor sections from studied mice confirmed their levels of VEGFR expression (1). The small blood vessels of the kidneys also appeared to contain a measurable level of VEGFR2. The authors suggested that the good correlation between in vivo PET and ex vivo results indicated that PET imaging with ^64^Cu-DOTA-VEGF_121_ could show the VEGFR expression level in vivo.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2864Cu-VEGF%29%20OR%20%28Vascular%20Endothelial%20Growth%20Factor%20for%20PET%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2864Cu-VEGF%29%20OR%20%28Vascular%20Endothelial%20Growth%20Factor%20for%20PET%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2864Cu-VEGF%29%20OR%20%28Vascular%20Endothelial%20Growth%20Factor%20for%20PET%29%29%20AND%20human)]

On the basis of microPET quantification data of biodistribution and pharmacokinetics of ^64^Cu-DOTA-VEGF_121_ in rats, Cai et al. (1) estimated the radiation dosimetry in normal human organs. The radioactivity distribution in rats was similar to that in mice. ^64^Cu-DOTA-VEGF_121_ was primarily excreted by the liver. Only the blood, liver, and kidneys exhibited high levels of radioactivity. No appreciable activity was observed in the urinary bladder at any time point. This suggested that ^64^Cu-DOTA-VEGF_121_ had a very slow renal clearance, and that the radioactivity bound in the kidney was not excreted. The kidney was the critical organ with the highest estimated radiation-absorbed dose of 1.05 ± 0.27 mGy/MBq (3.87 ± 1.01 rad/mCi). The liver dose was estimated to be 0.12 ± 0.02 mGy/MBq (0.43 ± 0.07 rad/mCi). The whole-body absorbed dose was estimated to be 0.05 ± 0.01 mGy/MBq (0.19 ± 0.02 rad/mCi).

## NIH Support

NIH NIBIB R21 EB001785, NCI R21 CA102123, NCI In Vivo Cellular Molecular Imaging Center Grant P50 CA114747, NCI Small Animal Imaging Resource Program Grant R24 CA93862, NCI Centers of Cancer Nanotechnology Excellence Grant 1U54CA119367-01.

## References

1 Cai W., Chen K., Mohamedali K.A., Cao Q., Gambhir S.S., Rosenblum M.G., Chen X. (2006). PET of Vascular Endothelial Growth Factor Receptor Expression. J Nucl Med.
2 Shinkaruk S., Bayle M., Lain G., Deleris G. (2003). Vascular endothelial cell growth factor (VEGF), an emerging target for cancer chemotherapy. Curr Med Chem Anticancer Agents.
3 Ranieri G., Patruno R., Ruggieri E., Montemurro S., Valerio P., Ribatti D. (2006). Vascular endothelial growth factor (VEGF) as a target of bevacizumab in cancer: from the biology to the clinic. Curr Med Chem.
4 Jain R.K. Tumor angiogenesis and accessibility: role of vascular endothelial growth factor Semin Oncol 2002 29Suppl 166 3 9 12516032
5 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
6. Laking, G.R. and P.M. Price, Positron emission tomographic imaging of angiogenesis and vascular function. Br J Radiol, 2003. 76 Spec No 1: p. S50-9.
7 Blankenberg F.G., Mandl S., Cao Y.A., O'Connell-Rodwell C., Contag C., Mari C., Gaynutdinov T.I., Vanderheyden J.L., Backer M.V., Backer J.M. (2004). Tumor imaging using a standardized radiolabeled adapter protein docked to vascular endothelial growth factor. J Nucl Med.
8 Cai W., Wu Y., Chen K., Cao Q., Tice D.A., Chen X. (2006). In vitro and In vivo Characterization of 64Cu-Labeled AbegrinTM, a Humanized Monoclonal Antibody against Integrin {alpha}v{beta}3. Cancer Res.